# 4-[^11^C]Methylphenyl-1,4-diazabicyclo[3.2.2]nonane-4-carboxylate

Chemical name: | 4-[^11^C]Methylphenyl-1,4-diazabicyclo[3.2.2]nonane-4-carboxylate
Abbreviated name: | [^11^C]CHIBA-1001
Synonym:
Agent category: | Compound
Target: | Neuronal α7 nicotinic acetylcholine receptor (nAChR)
Target category: | Receptor
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CHIBA-1001)]

Neuronal α4β2 nicotinic cholinergic receptors (nAChRs) are part of a heterogeneous family of ligand-gated ion channels expressed in the central nervous system, where their activation by acetylcholine and nicotine causes a rapid increase in cellular permeability to ions, such as Na^+^ and Ca^2+^ (1-3). Nicotinic receptors exist as pentamers (homomeric or heteromeric) in various brain regions and ganglia. There are nine subtypes of ligand-binding α receptors (α2 to α10) and four subtypes of structural β receptors (β2 to β5). nAChRs have been found to be involved in cognitive processes such as learning memory and control of movement in normal subjects. nAChR dysfunction has been implicated in a number of human diseases such as schizophrenia, Huntington's disease, Alzheimer's disease, and Parkinson's disease. nAChRs also play a significant role in nicotine addiction and other health problems associated with tobacco smoking.

3-[2(S)-2-Azetidinylmethoxy]pyridine (A-85380) is a highly potent and selective α4β2 nAChR agonist with subnanomolar affinity (4, 5). 6-[^18^F]Fluoro-A-85380 and 2-[^18^F]fluoro-A-85380 have been studied in humans as positron emission tomography (PET) agents for α4β2 nAChR imaging in the brain. A-85380 has also been labeled as 5-[^123^I]iodo-A-85380, which has been developed as a single-photon emission computed tomography agent for the non-invasive study of α4β2 nAChR in the brain. There are some implications that homomeric α7 nAChRs may play a role in the pathophysiology of neuropsychiatric disorders (6-8). α7 nAChRs are highly expressed in the cerebral cortex, hippocampus and subcortical limbic regions, which are involved in learning, memory, and information processing. 4-Bromophenyl-1,4-diazabicyclo[3.2.2]nonane-4-carboxylate (SSR180711) has been shown to be a potent and selective partial agonist for α7 nAChRs with nanomolar affinity (9). 4-[^11^C]Methylphenyl-1,4-diazabicyclo[3.2.2]nonane-4-carboxylate ([^11^C]CHIBA-1001), a 4-methyl substituted derivative of SSR180711, has been developed as a PET agent for the non-invasive study of α7 nAChR in the brain (10).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=nicotinic%20acetylcholine%20receptor+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (α7 nAChR (http://www.ncbi.nlm.nih.gov/gene/1139))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/118511)
- Clinical trials (α 7 nAChR (http://www.clinicaltrials.gov/ct2/results?term=alpha+7+nicotinic+cholinergic+receptors))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CHIBA-1001%20and%20synthesis)]

Hashimoto et al. (10) reported the synthesis of [^11^C]CHIBA-1001 by methylation of 4-(tributylstannyl)phenyl-1,4-diazabicyclo[3.2.2]nonane-4-carboxylate in the presence of CuCl_2_, potassium carbonate, and [^11^C]methyl iodide in DMF solution. The mixture was heated for 5 min at 70°C, and [^11^C]CHIBA-1001 was purified with high-performance liquid chromatography. Average radiochemical yield was 9.49 ± 1.45%. The radiochemical purity was >98% with a specific activity of 344 ± 36 GBq/µmol (9.3 ± 1.0 Ci/µmol; n = 12) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CHIBA-1001%20and%20in%20vitro)]

Hashimoto et al. (10) reported that CHIBA-1001 and SSR180711 exhibited IC_50_ values (obtained with the use of [^125^I]α-bungarotoxin) of 24.9 and 45.8 nM in rat brain membranes, respectively. CHIBA-1001 exhibited little affinity for α4β2, α2β4, and α3β4 nAChRs as well as other receptors.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CHIBA-1001%20and%20rodentia)]

Toyohara et al. (11) performed ex vivo biodistribution of [^11^C]CHIBA-1001 in normal mice (n = 4/group) at 1 – 90 min. The highest uptake (percentage of injected dose per gram of tissue: %ID/g) of [^11^C]CHIBA-1001 was found in the lungs (23.77) followed by the kidneys (13.17), liver (17.32), pancreas (9.15), spleen (5.44), small intestines (4.23), heart (6.16), brain (5.83) and muscle (2.46) at 1 -30 min after injection. The radioactivity level of [^11^C]CHIBA-1001 was low in the blood (0.65) at 5 min after injection. HPLC analysis of the plasma showed that 43.6% and 21.3% of [^11^C] CHIBA-1001 were intact at 15 and 30 min after injection with two major hydrophilic metabolites. On the other hand, little degradation of [^11^C] CHIBA-1001 was detected in the brain (>99% intact) at these time points. The effective dose estimated for human adults was 3.8 µSv/MBq. No blocking studies were reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CHIBA-1001%20and%20(dog%20or%20pig%20or%20sheep%20or%20rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CHIBA-1001%20and%20(primate%20not%20human))]

[^11^C]CHIBA-1001 PET studies with monkeys (n = 3) showed substantial brain accumulation with selective uptake in the regions of the hippocampus, cortex and basal ganglia (0.035-0.041%dose/cc)10–30 min after injection with gradual washouts (10); the cerebellum (0.022%dose/cc) showed lower binding than the other brain regions. [^11^C]CHIBA-1001 radioactivity in the brain regions was reduced to <0.028%dose/cc by pretreatment with the α7 nAChR agonists SSR180711 and A844606 (5.0 mg/kg, 30 min). However, the accumulation of radioactivity in the brain regions after administration of [^11^C]CHIBA-1001 was not affected by pretreatment with the selective α4β2 nAChR agonist A-85380 (1.0 mg/kg, 30 min). The fraction of unchanged [^11^C]CHIBA-1001 in the plasma as determined with high-performance liquid chromatography was ~50% at 60 min after injection.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CHIBA-1001%20and%20human)]

[^11^C]CHIBA-1001 (680 MBq/18.4 mCi, 17 nmol) PET scans with one healthy male subject (48 years old) showed substantial brain accumulation with selective uptake in the regions of the hippocampus, frontal cortex, thalamus, and cerebellum at 10–30 min after injection with gradual washouts (11). In Logan graphical analysis (total distribution volume, V_T_), the cerebellum (16.8 ml/g) showed lower binding than the thalamus (21.6 ml/g), amygdale (20.3), putamen (20.0 ml/g), hippocampus (19.7 ml/g), and frontal cortex (18.1 ml/g). The fraction of unchanged [^11^C]A-582941 in the plasma as determined with high-performance liquid chromatography was 92.2% at 30 min and 81.4% at 60 min after injection.

## References

1 Alkondon M., Albuquerque E.X. (2004). The nicotinic acetylcholine receptor subtypes and their function in the hippocampus and cerebral cortex. Prog Brain Res.
2 Gotti C., Riganti L., Vailati S., Clementi F. (2006). Brain neuronal nicotinic receptors as new targets for drug discovery. Curr Pharm Des.
3 Hogg R.C., Raggenbass M., Bertrand D. (2003). Nicotinic acetylcholine receptors: from structure to brain function. Rev Physiol Biochem Pharmacol.
4 Abreo M.A., Lin N.H., Garvey D.S., Gunn D.E., Hettinger A.M., Wasicak J.T., Pavlik P.A., Martin Y.C., Donnelly-roberts D.L., Anderson D.J., Sullivan J.P., Williams M., Arneric S.P., Holladay M.W. (1996). Novel 3-Pyridyl ethers with subnanomolar affinity for central neuronal nicotinic acetylcholine receptors. J Med Chem.
5 Sullivan J.P., Donnelly-Roberts D., Briggs C.A., Anderson D.J., Gopalakrishnan M., Piattoni-Kaplan M., Campbell J.E., McKenna D.G., Molinari E., Hettinger A.M., Garvey D.S., Wasicak J.T., Holladay M.W., Williams M., Arneric S.P. (1996). A-85380 [3-(2(S)-azetidinylmethoxy) pyridine]: in vitro pharmacological properties of a novel, high affinity alpha 4 beta 2 nicotinic acetylcholine receptor ligand. Neuropharmacology.
6 Gotti C., Zoli M., Clementi F. (2006). Brain nicotinic acetylcholine receptors: native subtypes and their relevance. Trends Pharmacol Sci.
7 Nomikos G.G., Schilstrom B., Hildebrand B.E., Panagis G., Grenhoff J., Svensson T.H. (2000). Role of alpha7 nicotinic receptors in nicotine dependence and implications for psychiatric illness. Behav Brain Res.
8 Nordberg A. (2001). Nicotinic receptor abnormalities of Alzheimer's disease: therapeutic implications. Biol Psychiatry.
9 Biton B., Bergis O.E., Galli F., Nedelec A., Lochead A.W., Jegham S., Godet D., Lanneau C., Santamaria R., Chesney F., Leonardon J., Granger P., Debono M.W., Bohme G.A., Sgard F., Besnard F., Graham D., Coste A., Oblin A., Curet O., Vige X., Voltz C., Rouquier L., Souilhac J., Santucci V., Gueudet C., Francon D., Steinberg R., Griebel G., Oury-Donat F., George P., Avenet P., Scatton B. (2007). SSR180711, a novel selective alpha7 nicotinic receptor partial agonist: (1) binding and functional profile. Neuropsychopharmacology.
10 Hashimoto K., Nishiyama S., Ohba H., Matsuo M., Kobashi T., Takahagi M., Iyo M., Kitashoji T., Tsukada H. (2008). [11C]CHIBA-1001 as a novel PET ligand for alpha7 nicotinic receptors in the brain: a PET study in conscious monkeys. PLoS ONE.
11 Toyohara J., Sakata M., Wu J., Ishikawa M., Oda K., Ishii K., Iyo M., Hashimoto K., Ishiwata K. (2009). Preclinical and the first clinical studies on [11C]CHIBA-1001 for mapping alpha7 nicotinic receptors by positron emission tomography. Ann Nucl Med.